# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid agouti-related protein-7C

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid agouti-related protein-7C
Abbreviated name: | ^64^Cu-DOTA-AgRP-7C
Synonym:
Agent Category: | Peptide
Target: | α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+peptides)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding (expressed as 50% inhibitory concentration (IC_50_)) to α_v_β_3_ (IC_50_, 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins. Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Only one cyclic RGD peptide, [^18^F]fluoropropionyl-galacto-c(-Arg-Gly-Asp-D-Phe-Lys) ([^18^F]-galacto-RGD), has been investigated for imaging expression of α_v_β_3_ integrin in cancer patients with tumors. However, [^18^F]-galacto-RGD has been shown to have low tumor accumulation and low signal/background ratios. Cystine knot peptides (knottins) share a common disulfide-bonded framework and a triple-stranded β-sheet fold (13). The integrin-binding RGD motif was grafted into a knottin from the trypsin inhibitor II of the squash plant (Ecballium elaterium) to form proteolytic resistant knottin peptides. Knottin 2.5D (with three disulfide-bonds) was identified from a series of genetically engineered knottin peptides to have nanomolar binding to the α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors (14, 15). Knottin 2.5D was labeled with N-succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB) to form 4-[^18^F]fluorobenzoyl-knottin 2.5D ([^18^F]FB-2.5D), which was evaluated for imaging tumor xenografts in mice with positron emission tomography (PET) (16). A truncated form of the agouti-related protein (AgRP), a 4-kDa knottin with four disulfide-bonds, was found to have high affinity for the α_v_β_3_ integrin (17). AgRP-7C peptide was identified using the yeast-displayed AgRP library. Jiang et al. (18) evaluated ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid agouti-related protein-7C (^64^Cu-DOTA-AgRP-7C) for PET imaging of α_v_β_3_ integrin expression in tumors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Knottin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Knottin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=841163))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AgRP-7C+synthesis)]

AgRP-7C was prepared with solid-phase peptide synthesis (18). The linear peptide was folded in the presence of 4 M guanidine, 10 mM reduced glutathione, 2 mM oxidized glutathione, and 0.5 M dimethylsulfoxide at pH 7.5. AgRP-7C was purified with high-performance liquid chromatography (HPLC). Peptide purity and molecular mass were confirmed with MALDI-TOF mass spectroscopy and HPLC. AgRP-7C was added to a mixture of DOTA, 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide, and N-hydroxysulfonosuccinimide (1:1:0.8 molar ratio) in water and incubated overnight at 4°C. DOTA-AgRP-7C was purified with HPLC. To label with ^64^Cu, DOTA-AgRP-7C was incubated with 37 MBq (1 mCi) ^64^CuCl_2_ in 0.1 N sodium acetate (pH, 5.5) for 1 h at 37°C. ^64^Cu-DOTA-AgRP-7C was purified with column chromatography with a radiochemical purity of >95% and a radiochemical yield of 46%. A specific activity of 4.29 GBq/µmol (58 mCi/µmol) was obtained at the end of synthesis. ^64^Cu-DOTA-AgRP-7C was 81% intact in mouse serum for up to 24 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AgRP-7C+in+vitro+studies)]

To determine the relative integrin-binding affinities (expressed as IC_50_ values) of AgRP, AgRP-7C, DOTA-AgRP-7C, and echistatin, a competition binding assay was performed with ^125^I-echistatin using U87MG human glioblastoma cells (18). The IC_50_ values for AgRP, AgRP-7C, DOTA-AgRP-7C, and echistatin were determined to be 1,400 ± 700, 20 ± 4, 14 ± 2, and 3.3 ± 0.6 nM, respectively. Cellular uptake of ^64^Cu-DOTA-AgRP-7C into U87MG cells was rapid with 4.6% of incubation dose at 60 min of incubation at 37°C. The uptake was inhibited 80% with excess c(RGDyK).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AgRP-7C+rodentia)]

Jiang et al. (18) performed ex vivo biodistribution studies of ^64^Cu-DOTA-AgRP-7C in nude mice (n = 3/group) bearing U87MG xenografts at 0.5, 2, and 4 h after intravenous injection. Tumor uptake values were 1.9 ± 0.5% injected dose per gram (ID/g), 2.7 ± 0.9%ID/g, and 1.9 ± 0.4% ID/g at 0.5, 2, and 4 h after injection, respectively. The organ with the highest radioactivity at 2 h after injection was the kidney (60% ID/g), followed by the liver (1.7% ID/g), stomach (1.4% ID/g), intestine (1.4% ID/g), and lung (1.2% ID/g). The radioactivity in the blood at 2 h after injection was <0.5% ID/g. The tumor/blood and tumor/muscle ratios were 6.6 and 17.2 at 2 h after injection, respectively. Co-administration of excess c(RGDyK) decreased tumor accumulation by 64% at 2 h after injection (P < 0.05), whereas little inhibition was observed in the kidney and other non-targeted tissues.

PET analysis was performed in nude mice bearing U87MG tumors after intravenous injection of ~2.22 MBq (60 μCi) ^64^Cu-DOTA-AgRP-7C. Tumors were clearly visualized at 0.5–24 h along with the kidneys. Tumor accumulation was determined to be 1.5% ID/g at 1 min after injection and 3.8% ID/g at 35 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AgRP-7C%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AgRP-7C+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AgRP-7C+Human+Studies)]

No references are currently available.

## NIH Support

5K 01 CA104706, 5R01 CA119053, R25 CA118681, P50 CA114747

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Pallaghy P.K., Nielsen K.J., Craik D.J., Norton R.S. (1994). A common structural motif incorporating a cystine knot and a triple-stranded beta-sheet in toxic and inhibitory polypeptides. Protein Sci.
14 Kimura R.H., Levin A.M., Cochran F.V., Cochran J.R. (2009). Engineered cystine knot peptides that bind alphavbeta3, alphavbeta5, and alpha5beta1 integrins with low-nanomolar affinity. Proteins.
15 Kimura R.H., Cheng Z., Gambhir S.S., Cochran J.R. (2009). Engineered knottin peptides: a new class of agents for imaging integrin expression in living subjects. Cancer Res.
16 Miao Z., Ren G., Liu H., Kimura R.H., Jiang L., Cochran J.R., Gambhir S.S., Cheng Z. (2009). An engineered knottin peptide labeled with 18F for PET imaging of integrin expression. Bioconjug Chem.
17 Jackson P.J., McNulty J.C., Yang Y.K., Thompson D.A., Chai B., Gantz I., Barsh G.S., Millhauser G.L. (2002). Design, pharmacology, and NMR structure of a minimized cystine knot with agouti-related protein activity. Biochemistry.
18 Jiang L., Kimura R.H., Miao Z., Silverman A.P., Ren G., Liu H., Li P., Gambhir S.S., Cochran J.R., Cheng Z. (2010). Evaluation of a (64)Cu-labeled cystine-knot peptide based on agouti-related protein for PET of tumors expressing alphavbeta3 integrin. J Nucl Med.